# Sialyl-Lewis^x^-liposome-Cy5.5

Chemical name: | Sialyl-Lewis^x^-liposome-Cy5.5
Abbreviated name: | SLX-Lipo-Cy5.5
Synonym:
Agent category: | Carbohydrate
Target: | E-selectin
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal/contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=34420911), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4506870) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6401) for more information about E-selectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SLX-Lipo)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging.

E-selectin is found on the cell surface of endothelial cells (3, 4). It binds to the carbohydrate moiety Sialyl-Lewis^x^ (SLX) on the cell surface of leukocytes. Tumor necrosis factor α and interleukin-1, released as a result of inflammatory stimuli, upregulate E-selectin and other adhesion molecule expression on the vascular endothelial cells, leading to leukocyte adhesion to the activated endothelium. E-selectin and other selectins are involved in arresting leukocytes on the endothelium. Hirai et al. (5) have developed liposomes containing SLX tetrasaccharides and Cy5.5-conjugated human serum albumin (SLX-Lipo-Cy5.5) for noninvasive magnetic resonance imaging of E-selectin expression in inflammation and tumor tissue. Cy5.5 is a NIR fluorescence dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SLX-Lipo%20and%20rodentia)]

Hirai et al. (5) reported the preparation of SLX-Lipo-Cy5.5. In brief, 20 mg human serum albumin (HSA) and 2 mg Cy5.5-NHS ester were dissolved in 3 ml of tris(hydroxymethyl)methylaminopropanesulfonic acid buffer (TAPS, pH 8.4) and incubated for 3 h at 37°C to form Cy5.5-HSA. There were ~3 Cy5.5 dye molecules per HSA molecule. Cy5.5-HSA was added to a solution of micelle suspension of dipalmitoylphosphatidylcholine (16.8 mg), cholesterol (10.1 mg), diacetylphosphate (1.8 mg), ganglioside (14.6 mg), dipalmitoylphosphatidylethanolamine (2.3 mg), and sodium cholate (46.9 mg) dissolved with 3 ml of chloroform/methanol (1:1, v/v) solution. The resulting Cy5.5-liposomes were further modified to incorporate SLX on the liposome surface with 3,3-dithiobis(sulfosuccinimidylpropionate) (DTSSP). DTSSP was used as a carbohydrate cross-linking reagent. DTSSP (10 mg) was added to 10 ml liposome solution and stirred for 2 h at 20–25°C, and further stirred overnight at 4°C. SLX (2 mg) was dissolved in 0.5 ml distilled water. NH_4_HCO_3_ (0.25 g) was added to the mixture and stirred for 3 days at 37°C. The aminated SLX was added to the liposome solution for conjugation to the liposome surface. SLX-Lipo-Cy5.5 was purified with ultrafiltration. The preparation of liposomes without SLX (Lipo-Cy5.5) was similar to the preparation of liposomes with SLX-Lipo-Cy5.5. Binding of N-acetyllactosamine (G4GN) on the liposome surface was prepared in a manner similar to that for G4GN-Lipo-Cy5.5 binding as sugar control liposomes.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SLX-Lipo%20and%20in%20vitro)]

Lipid and protein content of SLX-Lipo-Cy5.5 was 3.7 and 1.2 mg/ml, respectively (5). For Lipo-Cy5.5, 3.8 mg/ml lipid and 1 mg/ml protein content were obtained. The average liposome size was ~100 nm with a zeta potential of -40 mV (negatively charged liposome surface). The preparations were stable for 6 months at 4°C. No analytical data of the stoichiometry of the liposome components (SLX and Cy5.5) was provided.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SLX-Lipo%20and%20rodentia)]

Hirai et al. (5) used antibodies against type II collagen and lipopolysaccharide to induce arthritis in mice. NIR fluorescence imaging was performed on the inflamed hind leg of each mouse before and after intravenous injection of SLX-Lipo-Cy5.5, Lipo-Cy5.5, or G4GN-Lipo-Cy5.5. Accumulation of SLX-Lipo-Cy5.5 in the inflammation region as measured with fluorescence imaging was higher than either Lipo-Cy5.5 or G4GN-Lipo-Cy5.5 at 24 h after injection. Scanning fluorescent microscopy of the blood vessels and the surrounding tissues of the inflammation region showed that SLX-Lipo-Cy5.5 adhered to the blood vessels at 6 h after injection and shifted to the surrounding tissue by 24 h, with peak accumulation at 48 h. On the other hand, the accumulation of Lipo-Cy5.5 or G4GN-Lipo-Cy5.5 in the surrounding tissue was lower than that of SLX-Lipo-Cy5.5. Minaguchi et al. (6) showed that histological immunofluorescence of E-selectin on endothelial cells of the inflamed region colocalized with SLX-Lipo-Cy5.5.

NIR fluorescence imaging showed that SLX-Lipo-Cy5.5 accumulated in the tumor region in mice bearing Ehrlich ascites tumor cells at 24 h, with peak accumulation at 48 h (5). On the other hand, Lipo-Cy5.5 or G4GN-Lipo-Cy5.5 did not show any accumulation in the tumor region. SLX-Lipo-Cy5.5 whole-body NIR fluorescence imaging showed strong fluorescence signals from the liver, urinary bladder, and tumor region at 96 h after injection. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SLX-Lipo%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SLX-Lipo%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SLX-Lipo%20and%20human)]

No publication is currently available.

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Bird M.I., Foster M.R., Priest R., Malhotra R. (1997). Selectins: physiological and pathophysiological roles. Biochem Soc Trans.
4 Rosen S.D., Bertozzi C.R. (1994). The selectins and their ligands. Curr Opin Cell Biol.
5 Hirai M., Minematsu H., Kondo N., Oie K., Igarashi K., Yamazaki N. (2007). Accumulation of liposome with Sialyl Lewis X to inflammation and tumor region: application to in vivo bio-imaging. Biochem Biophys Res Commun.
6 Minaguchi J., Oohashi T., Inagawa K., Ohtsuka A., Ninomiya Y. (2008). Transvascular accumulation of Sialyl Lewis X conjugated liposome in inflamed joints of collagen antibody-induced arthritic (CAIA) mice. Arch Histol Cytol.